# N-[N-[(S)-1,3-Dicarboxypropyl]carbamoyl]-S-[^11^C]methyl-L-cysteine

Use this form to tell us important information about this document, then start the text on the following page. All information you give in this form will appear in the document.

Chemical name: | N-[N-[(S)-1,3-Dicarboxypropyl]carbamoyl]-S-[^11^C]methyl-L-cysteine
Abbreviated name: | [^11^C]DCMC
Synonym: | [^11^C]MCG
Agent Category: | Amino acid
Target: | Prostate-specific membrane antigen (PSMA)
Target Category: | Binding to PSMA
Method of detection: | PET
Source of signal: | ^11^C
Activation: | No
Studies: | - In vitro; - Rodents; - Non-human primates | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=DCMC%5BAll%20Fields%5D)]

The prostate-specific membrane antigen (PSMA) is a cell-surface glycoprotein with a molecular weight of ~100 kDa. It is expressed predominantly in the prostate and has also been detected in other tissues such as the kidney, the proximal small intestine, and the salivary glands. Minimal expression has also been observed in the brain (1). It is believed that PSMA plays an important role in the progression of prostate cancer, glutamatergic neurotransmission, and in the absorption of folate (2). This glycoprotein is specifically upregulated several-fold in prostate cancers (PCAs), metastatic disease, and hormone-refractory PCAs because androgen levels inversely modulate PSMA levels (3). Interestingly, PSMA also has an elevated expression in the neovasculature of solid tumors, but is absent in normal neovasculature and prostate cancers tumors (4). Although its function in the prostate is unknown, in the central nervous system PSMA metabolizes N-acetyl-aspartyl-glutamate (NAAG), and in the proximal small intestine it removes γ-linked glutamates from poly-γ-glutamate folate and folate hydrolase (FOLH1), and also acts as a carboxypeptidase, glutamate carboxypaptidase II (GCPII) (1). Due to its unique distribution, PSMA can be used as a marker for the detection of metastatic cancers with imaging agents. Although a commercially available monoclonal antibody [^111^In-Capromomab pendetide (ProstaScint)] is in clinical use for the detection of prostate cancer, the results obtained with this antibody are not entirely reliable (5). In addition, the antibodies have limited access to tumors and may produce low signal-to-noise ratios because the target is intracellular, whereas PSMA is present on the cell surface (6, 7). Therefore, a small molecule ^11^C ligand, N-[N-[(S)-1,3-dicarboxypropyl]carbamoyl]-S-[^11^C]methyl-L-cysteine ([^11^C]DCMC), was synthesized and evaluated for the imaging of PSMA-positive and -negative tumors using positron emission tomography (PET) in an in vivo rodent model for prostate cancer (8).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=DCMC%20AND%20synthesis)]

N-[N-[(S)-1,3-Dicarboxypropyl]carbamoyl]-L-cysteine was used as a precursor for the synthesis of [^11^C]DCMC (9, 10). The precursor (9) was dissolved in N,N-dimethylformamide (DMF), and a fresh DMF/ammonia solution was added to the solution and then followed by water (10). The solution was cooled to 20^o^C and ^11^C-labeled iodomethane was bubbled through it. The reaction contents were subsequently heated for 60 seconds in a 45^o^C bath, and the reaction was terminated with acetonitrile/water/trifluoroacetic acid (6:94:0.075), followed by the addition of 20% trifluoroacetic acid (10). [^11^C]DCMC was separated by high-performance liquid chromatography, reformulated in 0.9% saline, and sterile filtered. The specific radioactivity of [^11^C]DCMC was determined and sterile sodium bicarbonate was added to the radioactive compound to bring the pH of the final formulation to ~7.0. The time for synthesis, including formulation, was ~30 min. Based on the amount of ^11^C-labeled iodomethane used for the synthesis, the yield of [^11^C]DCMC was calculated to be 16% at the end of synthesis, with a purity of >97% (10) and specific radioactivity of 167 Gbq/µmol (4,000 Ci/mmol) within 30 min after bombardment.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=DCMC%20AND%20in%20vitro)]

The relative affinity of DCMC for PSMA was determined using the NAAG peptidase assay in membranes isolated from Chinese hamster ovary cells transfected with rat GCPII (11). For this assay, 4 µmol/L NAAG that contained trace amounts of ^3^H-NAAG was incubated with the membranes in the presence of 0.1, 0.3, 1, 3, 10, 30, 100, 300, and 1,000 nmol/L DCMC. The NAAG hydrolysis product was separated by ion-exchange chromatography and determined by scintillation spectrophotometry (8). The K_i_ of DCMC for the NAAG activity was determined to be 1.9 nmol/L.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=DCMC%20and%20rodentia)]

The in vivo biodistribution of [^11^C]DCMC was investigated in healthy (10) and xenograft-bearing mice (8).

Male CD-1 mice weighing 20 to 25 g received an injection of 100 µCi (3700 kBq) [^11^C]DCMC in 200 µl saline through the tail vein (12). The mice were killed 5, 15, 30, 60, and 120 minutes after the injection. Brains were removed from the animals, and the cerebellum, olfactory bulb, hypothalamus, hippocampus, striatum, parietal cortex, brainstem, and the thalamus were harvested. The various tissues were weighed and the radioactivity was determined with an automated γ counter. For binding specificity, the mice were pretreated with doses of 1, 10, and 100 mg/kg 2-(phosphonomethyl)pentanedioic acid (PMPA), a potent inhibitor of GCPII (12), 5 minutes prior to the injection of [^11^C]DCMC. The uptake of [^11^C]DCMC was highest (61.0% of total) in the kidneys (which also have the highest GCPII concentration in the body) and was completely washed out by 120 minutes after administration. The prostate had a maximum of 2.55% uptake, probably because the mouse prostate has low levels of PSMA (10, 13). In this study, the brain, cerebellum, hippocampus, and cortex showed minimal incorporation of radioactivity. A target binding specificity of [^11^C]DCMC was indicated because excess unlabelled DCMC or PMPA (up to 1 mg/kg) blocked uptake in the kidneys (10). In this study, the metabolites were determined at 5,15, 30, and 60 minutes after administration. The plasma and kidneys showed the highest metabolite levels, 9.2% and 10.4% of the total, respectively, at 60 minutes. This is probably because the metabolites bind to and are excreted through the kidneys.

The human LNCaP cell line (PSMA-positive) of human prostate cancer was used to develop the xenograft-bearing mouse (8). For PSMA-negative controls, animals with PC-3 (prostate cancer) and MCF-7 (breast cancer) cell xenografts were used. For the study, animals bearing xenografts (17–20 g) were injected through the tail vein either with 6.49 pmol, 200 µCi (7400 kBq) [^11^C]DCMC alone or in combination with 50 mg/kg PMPA. Blood was collected immediately after animals were killed; select tissues were harvested and weighed, and absorbed radioactivity was counted in a γ counter. The biodistribution of [^11^C]DCMC was highest in the LNCaP tumors, and tumors with MCF-7 or PC-3 cells exhibited significantly lower incorporation of radioactivity (8). Using excess amounts of PMPA as a blocking agent, these observations were confirmed with PET and planer γ scintigraphy imaging studies, respectively. Similar observations, as described above, were made with imaging of the kidneys (8).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=DCMC%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No publications are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=DCMC%20AND%20Primates)]

Renal cortical uptake and clearance studies of [^11^C]DCMC were performed using PET in an ~30-kg adult male baboon, Papio Anubis (10). PET scanning was initiated immediately after an intravenous injection of 10 mCi (370 MBq) high specific activity [^11^C]DCMC. Thirty-five simultaneous, contiguous, sequential, high-resolution quantitative tomographic slices of the brain were obtained over a 90-minute period. In addition, the animal was positioned so that the renal cortex was in complete view. This study showed there was significant uptake of [^11^C]DCMC in the renal cortex of the animal, which was decreased by pretreatment with 2 mg/kg PMPA. Uptake of [^11^C]DCMC in the brain was low and the authors concluded that [^11^C]DCMC is not suitable to measure GCPII activity in the brain.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20human)]

No publications are currently available.

## References

1 Ghosh A, Heston WD. (2004). Tumor target prostate specific membrane antigen (PSMA) and its regulation in prostate cancer. J Cell Biochem.
2. O'Keefe, D, D Bachich, and WD Heston, Prostate specific membrane antigen. Prostate cancer, biology, genetics, and the new therapeutics., ed. L Chung, W Issacs, and J Simons. 2001, New Jersey: Humana Press. 307-326.
3 Wright GL, Grob BM, Haley C, Grossman K, Newhall K, Petrylak D, Troyer J, Konchuba A, Schellhammer PF, Moriarty R. (1996). Upregulation of prostate-specific membrane antigen after androgen-deprivation therapy. Urology.
4 Chang SS. (2004). Monoclonal antibodies and prostate-specific membrane antigen. Curr Opin Investig Drugs.
5 Ponsky LE, Cherullo EE, Starkey R, Nelson D, Neumann D, Zippe CD. (2002). Evaluation of preoperative ProstaScint scans in the prediction of nodal disease. Prostate Cancer Prostatic Dis.
6 Jain RK. (1999). Transport of molecules, particles, and cells in solid tumors. Annu Rev Biomed Eng.
7 Sundaresan G, Yazaki PJ, Shively JE, Finn RD, Larson SM, Raubitschek AA, Williams LE, Chatziioannou AF, Gambhir SS, Wu AM. (2003). 124I-labeled engineered anti-CEA minibodies and diabodies allow high-contrast, antigen-specific small-animal PET imaging of xenografts in athymic mice. J Nucl Med.
8 Foss CA, Mease RC, Fan H, Wang Y, Ravert HT, Dannals RF, Olszewski RT, Heston WD, Kozikowski AP, Pomper MG. (2005). Radiolabeled small-molecule ligands for prostate-specific membrane antigen: in vivo imaging in experimental models of prostate cancer. Clin Cancer Res.
9 Kozikowski AP, Nan F, Conti P, Zhang J, Ramadan E, Bzdega T, Wroblewska B, Neale JH, Pshenichkin S, Wroblewski JT. (2001). Design of remarkably simple, yet potent urea-based inhibitors of glutamate carboxypeptidase II (NAALADase). J Med Chem.
10 Pomper MG, Musachio JL, Zhang J, Scheffel U, Zhou Y, Hilton J, Maini A, Dannals RF, Wong DF, Kozikowski AP. (2002). 11C-MCG: synthesis, uptake selectivity, and primate PET of a probe for glutamate carboxypeptidase II (NAALADase). Mol Imaging.
11 Fuhrman S, Palkovits M, Cassidy M, Neale JH. (1994). The regional distribution of N-acetylaspartylglutamate (NAAG) and peptidase activity against NAAG in the rat nervous system. J Neurochem.
12 Jackson PF, Cole DC, Slusher BS, Stetz SL, Ross LE, Donzanti BA, Trainor DA. (1996). Design, synthesis, and biological activity of a potent inhibitor of the neuropeptidase N-acetylated alpha-linked acidic dipeptidase. J Med Chem.
13 Tiffany CW, Lapidus RG, Merion A, Calvin DC, Slusher BS. (1999). Characterization of the enzymatic activity of PSM: comparison with brain NAALADase. Prostate.